# ^67^Ga labeled cyclic diethylenetriamine pentaacetic acid Insulin

Chemical name: | ^67^Ga-Labeled cyclic diethylenetriamine pentaacetic acid insulin
Abbreviated name: | [^67^Ga]-Insulin
Synonym:
Agent Category: | Protein
Target: | Insulin receptor
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of Signal/Contrast: | ^67^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=386828) and nucleotide (http://www.nature.com/nature/journal/v282/n5738/abs/282525a0.html) sequence of human insulin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=insulin+)]

Although the main role of insulin is considered to be the regulation of glucose transport and metabolism, insulin is known to influence directly or indirectly a variety of other metabolic processes in the cell such as protein synthesis, DNA transcription, and RNA translation in that insulin receptors are found in almost all cell types (1). Because insulin plays a key role in the regulation of these important processes, it has been associated with conditions such as diabetes, obesity, heart disease, neurodegenerative diseases, and even cancer (2-5). The insulin amino acid sequence appears to be well conserved throughout the animal kingdom, and there is a difference of less than five amino acids between the human, bovine, and porcine molecules. In addition, insulin from these mammals is known to have an invariant location of three disulfide bonds (6). Insulin was initially purified mainly from bovine and porcine sources for the treatment of humans, but because of high demand insulin is now available commercially as a recombinant form expressed in either Escherichia coli or yeast cells (7). Insulin is approved by the United States Food and Drug Administration for the treatment of diabetes and is being evaluated in several diabetes-related clinical trials (http://clinicaltrials.gov/ct2/results?term=insulin).

Insulin mediates its effects through the activation of a receptor tyrosine kinase that has been studied primarily in cultured cells or in isolated cell membranes (1). Radioactive iodine (^123^I) was used to label insulin, and the in vivo metabolism of this radiolabeled molecule has been studied in rodents and humans with the use of single-photon emission computed tomography (SPECT); however, ^123^I has a very short half-life (~13 h), making it of limited value in the investigation of changes in receptor densities that may occur under various pathological conditions (8-10). Positron emission tomography (PET) using insulin labeled with radioactive fluorine (^18^F) has been used to study insulin receptors in monkeys and under in vitro conditions in HEK-293 cells (11, 12). This labels also has a very short half-life (~110 min), therefore this limitation prohibits the use or either ^123^I or ^18^F labeled insulin in studies to investigate receptor changes over extended periods. Insulin labeled with meta-stable technetium (^99m^Tc) was also used to study the biodistribution in rats using SPECT, but this radionuclide also has a short half-life of ~6 h (13). Jalilian et al. used radioactive gallium (^67^Ga), which has a half-life of >3 days, to label insulin, and these investigators used SPECT to study its biodistribution in normal rats (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=67Ga+insulin)]

The synthesis of ^67^Ga-labeled insulin was described by Jalilian et al. (14). Pharmaceutical-grade insulin was obtained from commercial sources and used without further purification. Cyclic diethylenetriamine pentaacetic acid (DTPA) was coupled to insulin as described elsewhere (15). For radiolabeling the DTPA-conjugated insulin, [^67^Ga]gallium chloride in 0.2 M hydrochloric acid was added to a conical vial and dried under a stream of nitrogen. The DTPA-insulin in phosphate buffer (pH 8.0) was added to the vial and mixed gently for 30 s. The resulting solution was then incubated at room temperature for 30 min, and the products were checked with instant thin-layer chromatography (ITLC) and high-performance liquid chromatography (HPLC). The Rf values for the various components on ITLC were not reported. If the purity of labeled insulin was <90%, it was purified with gel filtration on a Sephadex G-50 column. The specific activity of ^67^Ga-labeled insulin was reported to be 0.68–0.86 MBq/166 nmol (0.018–0.023 mCi/166 nmol). The radiochemical yield of the reaction was reported to be 99%; final purity of the product was not reported (15). The stability of ^67^Ga-labeled insulin was investigated in phosphate-buffered saline (PBS) containing human serum (pH 7.4) for up to 2 h at 37°C (15). No loss of radionuclide or change in ^67^Ga-labeled insulin was reported on exposure to human serum under these conditions as determined with ITLC or HPLC.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=67Ga+insulin+in+vitro)]

The in vitro binding activity of ^67^Ga-labeled insulin was studied in human white blood cells (14). Blood samples were obtained from fasting and non-fasting volunteers and centrifuged at 3,000 rpm for 5 min. The cell pellet was washed three times with PBS and gently resuspended in the same buffer. Radiolabeled insulin was added to the cell suspension, and the mixture was incubated at 37°C for up to 150 min. Cell samples were taken from the incubation mixture at different times and washed with PBS, and the bound radioactivity was determined. Blood cells from the non-fasting volunteers did not show any change in insulin binding over time. The investigators suggested that this was probably because the insulin secreted into the blood after eating competed with the labeled radiochemical. A higher binding of labeled insulin was observed in cells obtained from the fasting volunteers (14). The affinity and dissociation constants for ^67^Ga-labeled insulin and blocking studies using unlabeled insulin were not reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=67Ga+insulin+rodentia)]

The biodistribution of [^67^Ga]-labeled insulin was investigated in normal rats (14). The rats were injected with the radiolabeled compound through the tail vein, and the animals were euthanized 2–44 h after injection. The number of animals used per time point was not reported. All major organs of the animals were collected and weighed, and accumulated radioactivity was counted. SPECT imaging was performed on animals 24 and 48 h after the administration of ^67^Ga-labeled insulin. The radiolabel was reported to clear from the blood within 2–3 h, and the tracer accumulated primarily in the liver (>2.5% of the injected dose/gram tissue (% ID/g)), with a small fraction (<0.25% ID/g) accumulating in the spleen and kidneys. SPECT imaging revealed that radioactivity accumulated primarily in the liver, as reported earlier with ^123^I-labeled insulin (16). Blocking studies were not reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=67Ga+insulin+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=67Ga+insulin+humans)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Iozzo P., Osman S., Glaser M., Knickmeier M., Ferrannini E., Pike V.W., Camici P.G., Law M.P. (2002). In vivo imaging of insulin receptors by PET: preclinical evaluation of iodine-125 and iodine-124 labelled human insulin. Nucl Med Biol.
2 DeFronzo R.A. (1997). Insulin resistance: a multifaceted syndrome responsible for NIDDM, obesity, hypertension, dyslipidaemia and atherosclerosis. Neth J Med.
3 Hoyer S. (1998). Is sporadic Alzheimer disease the brain type of non-insulin dependent diabetes mellitus? A challenging hypothesis. J Neural Transm.
4 Kaaks R., Toniolo P., Akhmedkhanov A., Lukanova A., Biessy C., Dechaud H., Rinaldi S., Zeleniuch-Jacquotte A., Shore R.E., Riboli E. (2000). Serum C-peptide, insulin-like growth factor (IGF)-I, IGF-binding proteins, and colorectal cancer risk in women. J Natl Cancer Inst.
5 Paternostro G., Pagano D., Gnecchi-Ruscone T., Bonser R.S., Camici P.G. (1999). Insulin resistance in patients with cardiac hypertrophy. Cardiovasc Res.
6 Mohan V. (2002). Which insulin to use? Human or animal?. Current Science.
7 Bell D.S. (2007). Insulin therapy in diabetes mellitus: how can the currently available injectable insulins be most prudently and efficaciously utilised?. Drugs.
8 Dozio N., Micossi P., Galimberti G., Sartori S., Pozza G., Dosio F., Savi A., Gerundini P.G., Fazio F., Chiumello G., et al. (1992). In vivo demonstration of insulin-receptor defect with 123I-labeled insulin and scintigraphic scanning in severe insulin resistance. Diabetes Care.
9 Sodoyez J.C., Sodoyez-Goffaux F., Guillaume M., Merchie G. (1983). [123I]Insulin metabolism in normal rats and humans: external detection by a scintillation camera. Science.
10 Virgolini I., Angelberger P., Banyai M., Knobl P., Pantev T., Neuhold N., Prager R., Sinzinger H. (1991). 123I-tyrosine-(A14)-insulin: preparation and preliminary clinical studies. Wien Klin Wochenschr.
11 Eastman R.C., Carson R.E., Jacobson K.A., Shai Y., Channing M.A., Dunn B.B., Bacher J.D., Baas E., Jones E., Kirk K.L., et al. (1992). In vivo imaging of insulin receptors in monkeys using 18F-labeled insulin and positron emission tomography. Diabetes.
12 Guenther K.J., Yoganathan S., Garofalo R., Kawabata T., Strack T., Labiris R., Dolovich M., Chirakal R., Valliant J.F. (2006). Synthesis and in vitro evaluation of 18F- and 19F-labeled insulin: a new radiotracer for PET-based molecular imaging studies. J Med Chem.
13 Awasthi V., Gambhir S., Sewatkar A.B. (1994). 99mTc-insulin: labeling, biodistribution and scintiimaging in animals. Nucl Med Biol.
14 Jalilian A.R., Garosi J., Gholami E., Akhlaghi M., Saddadi F., Bolourinovin F., Karimian A. (2007). Evaluation of [67Ga]-insulin for insulin receptor imaging. Nucl Med Rev Cent East Eur.
15 Hnatowich D.J., Layne W.W., Childs R.L., Lanteigne D., Davis M.A., Griffin T.W., Doherty P.W. (1983). Radioactive labeling of antibody: a simple and efficient method. Science.
16 Sodoyez J.C., Sodoyez Goffaux F., von Frenckell R., De Vos C.J., Treves S., Kahn C.R. (1985). Differing effects of antiinsulin serum and antiinsulin receptor serum on 123I-insulin metabolism in rats. J Clin Invest.